# Gd-DOTA-G-NH(CH_2_)_11_CO-RSPAYYTAA-(CH_2_CH_2_O)_8_-R

Chemical name: | Gd-DOTA-G-NH(CH_2_)_11_CO-RSPAYYTAA-(CH_2_CH_2_O)_8_-R
Abbreviated name: | GdPCA2
Synonym: | PCA2-switch
Agent category: | Peptide
Target: | Matrix metalloprotein-2 (MMP-2)
Target category: | Enzyme
Method of detection: | Magnetic Resonance Imaging (MRI)
Source of signal/contrast: | Gadolinium
Activation: | Yes
Studies: | - In vitro; - Rodents | No structure is current available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=PCA2-switch)]

Matrix metalloproteinases (MMPs) are a family of zinc-dependent endopeptidases localized at the cell surface or in extracellular compartments (1). MMPs degrade all components of the extracellular matrix (ECM) and are associated with a variety of pathological conditions such as wound healing, tissue remodeling, tumor angiogenesis, and embryo development. The active site of MMPs contains a catalytic domain coordinated by zinc to recognize motifs with a consensus sequence of PXX↓X_Hy_, where ↓ represents the cleavage point and X_Hy_ represents a large hydrophobic residue (2). Excess MMP activity has been observed in conjunction with many diseases, including rheumatoid arthritis, osteoarthritis, autoimmune diseases, cardiovascular diseases, and cancer (3). For example, an overexpression of MMP subtype-2 (MMP-2 or gelatinase A), an enzyme that degrades type IV collagen and gelatin, is present in many human tumors (4). Thus, MMP has been an important therapeutic target for many years (5).

Gadolinium (Gd)-labeled DOTA-G-NH(CH_2_)_11_CO-RSPAYYTAA-(CH_2_CH_2_O)_8_-R (GdPCA2) is a proteinase-modulated contrast agent (PCA) for in vivo imaging of MMP-2 with magnetic resonance imaging (MRI) (6). GdPCA2 consists of four components: a peptide substrate (RSPAY↓YTAA) specific for MMP-2, a Gd-DOTA complex as an MRI probe, an alkyl chain of 12-carbon as a hydrophilic linker between the N-terminus of the peptide and the MRI probe, and an eight-unit polyethylene glycol (PEG_8_) chain linked to the C-terminus of the peptide to enhance the solubility of GdPCA2. The cleavage of GdPCA2 by MMP-2 produces a less soluble Gd^3+^-labeled fragment. Thus, the Gd species acts as a solubility switch specific for the enzyme MMP-2. GdPCA2 may have different pharmacokinetics than its cleaved product, which can be used to evaluate MMP-2 activity via dynamic MRI measurement.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( PCA2-switch)+AND+synthesis%0D%0A)]

Lebel et al. briefly described the preparation of GdPCA2 (6). With standard protocols of solid-phase peptide synthesis, the N-terminus of the PCA2 peptide (RSPAYYTAA) was linked to the Gd-DOTA via a 12-carbon alkyl chain, and the C-terminus of the peptide was linked to an amino PEG_8_-Arg to yield GdPCA2.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( PCA2-switch)+AND+%22in+vitro%22)]

The cleavage efficacy (k_cat_/K_m_) of GdPCA2 was measured in vitro (6). Cleavage of GdPCA2 by MMP-2 produced a free amino group that was detectable with the addition of fluorescamine. The k_cat_/K_m_ was 1.2 × 10^5^ M^-1^s^-1^ for GdPCA2, which was slightly lower than the k_cat_/K_m_ of 3.1 × 10^5^ M^-1^s^-1^ for the PCA2 peptide but 37.5 times higher than the k_cat_/K_m_ of 3.1 × 10^5^ M^-1^s^-1^ for a scrambled GdPCA2 (GdPCA2-scrambled) that contained a scrambled peptide (SYPATAYA). The cleaved products were further examined with high-performance liquid chromatography and mass spectrometry; two fragments were found for GdPCA2 (specific cleavage) and four fragments for GdPCA2-scrambled (non-specific cleavage).

The T_1_ relaxivity of GdPCA2 and its cleaved product (cleaved-GdPCA2) was measured at 7 T (6). The value for the GdPCA2 was 2.06 ± 0.03 mM^-1^s^-1^ in H_2_O and 2.03 ± 0.03 mM^-1^s^-1^ in aqueous bovine albumin (BSA) (14 mg/ml), respectively. The values for the cleaved-GdPCA2 were slightly higher: 2.18 ± 0.03 mM^-1^s^-1^ in H_2_O and 2.19 ± 0.02 mM^-1^s^-1^ in aqueous BSA. In comparison, the T_1_ relaxivity of GdDTPA was 3.58 ± 0.10 mM^-1^s^-1^.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( PCA2-switch) +AND++rodentia)]

Lebel et al. used GdPCA2 with dynamic contrast-enhanced MRI to examine the MMP-2 activity as a function of time (the pharmacokinetics) in vivo (6). Balb/c mice were implanted with two types of mammary carcinomas ~310 mm^3^ in volume: a wild-type MC7-L1 (WT) tumor that had overexpressed MMP-2 at the left hind limb and a knockdown MC7-L1 (KD) tumor that had suppressed MMP-2 (~51% lower) at the right hind limb. The tumor-bearing mice (n = 8) were injected with 2 μmol GdPCA2 via the caudal vein, and sequential T_1_-weighted images were collected at 7 T at a temporal resolution of 51 s. The signal in each voxel was converted into the relaxation rate difference (ΔR_1_) between the relaxation rate R_1_ and the precontrast relaxation rate R_1,0_. A rapid increase in ΔR_1_ was observed in the WT and KD tumors after the injection of GdPCA2, but the subsequent pharmacokinetics were different in the two types of tumors. In the WT tumor, ΔR_1_ remained constant 5–20 min after injection, then exhibited a second increase with a maximum at ~40 min. In the KD tumor, ΔR_1_ continued to decrease 5 min after injection. As a control, the tumor-bearing mice (n = 2) were injected with 2 μmol GdPCA2-scrambled and imaged with the same MRI protocols. A pharmacokinetics similar to that of the KD tumor after injection of GdPCA2 was observed in both the WT tumor and the KD tumor after injection of GdPCA2-scrambled. This result suggests that the GdPCA2 in WT tumors is different from the GdPCA2-scrambled in both tumors. In the WT tumor, the first increase in ΔR_1_ after injection of GdPCA2 was caused by the perfusion of GdPCA2 from the blood to the ECM, as seen in all tumors and/or injection with GdPCA2-scrambled; the second increase was attributed to the activation of enzyme MMP-2, which was only present in tumors overexpressing MMP-2 (WT type).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( PCA2-switch) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( PCA2-switch) +AND+human)]

No publication is currently available.

## References

1 Lepage M., Dow W.C., Melchior M., You Y., Fingleton B., Quarles C.C., Pepin C., Gore J.C., Matrisian L.M., McIntyre J.O. (2007). Noninvasive detection of matrix metalloproteinase activity in vivo using a novel magnetic resonance imaging contrast agent with a solubility switch. Mol Imaging.
2 Chen E.I., Kridel S.J., Howard E.W., Li W., Godzik A., Smith J.W. (2002). A unique substrate recognition profile for matrix metalloproteinase-2. J Biol Chem.
3 Yan C., Boyd D.D. (2007). Regulation of matrix metalloproteinase gene expression. J Cell Physiol.
4 Klein G., Vellenga E., Fraaije M.W., Kamps W.A., de Bont E.S. (2004). The possible role of matrix metalloproteinase (MMP)-2 and MMP-9 in cancer, e.g. acute leukemia. Crit Rev Oncol Hematol.
5 Overall C.M., Kleifeld O. (2006). Tumour microenvironment - opinion: validating matrix metalloproteinases as drug targets and anti-targets for cancer therapy. Nat Rev Cancer.
6 Lebel R., Jastrzebska B., Therriault H., Cournoyer M.M., McIntyre J.O., Escher E., Neugebauer W., Paquette B., Lepage M. (2008). Novel solubility-switchable MRI agent allows the noninvasive detection of matrix metalloproteinase-2 activity in vivo in a mouse model. Magn Reson Med.